# VHPKQHRGGSKGC-liquid perfluorocarbon nanoparticles

Chemical name: | VHPKQHRGGSKGC-liquid perfluorocarbon nanoparticles
Abbreviated name: | VCAM-1-targeted nanoparticles
Synonym:
Agent category: | Peptide
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | ^19^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VCAM-1+nanoparticle)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal.

Endothelial cells are important cells in inflammatory responses (2, 3). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (4).

VCAM-1 is found in very low amounts on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (5-9). VCAM-1 binds to very late antigen-4 (VLA-4) integrin on the cell-surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (10). Over-expression of VCAM-1 by atherosclerotic lesions plays an important role in their progression towards vulnerable plaques, which may erode and rupture. CLIO nanoparticles targeted with anti-VCAM-1 antibody are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (11). A linear peptide (VHPKQHR) homologous to VLA-4 bound to and was internalized by VCAM-1-expressing cells (12, 13). VHPKQHRGGSKGC was synthesized and conjugated to liquid perfluorocarbon (PFC) nanoparticles to form VCAM-1-targeted nanoparticles (14). MR imaging was performed utilizing the multiple ^19^F moieties for quantification.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VCAM-1+AND+micad%5Bbook%5D)
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=VCAM-1%5BAll+Fields%5D)
- Clinical trials (VCAM-1 (http://www.clinicaltrials.gov/ct2/results?term=VCAM-1))
- FDA Drug information (VCAM-1 (http://google2.fda.gov/search?q=vcam-1&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+synthesis)]

The synthesis of VCAM-1-targeted nanoparticles was described by Southworth et al. (14) Liquid PFC mixture comprised 20% (v/v) perfluoro-15-crown-5-ether (CE), 1.5% surfactant/lipid, 1.7% glycerine, and 0.135mol% rhodamine in water. N-[{w-[4-(p-maleimidophenyl)butanoyl]amino} poly(ethylene glycol)2000] 1,2-distearoyl-sn-glycero-3-phosphoethanolamine (MPB-PEG-DSPE) and VHPKQHRGGSKGC were added to the PFC emulsions in 1:1 molar ratio (0.09mol%) under nitrogen at 37°C. The mixture was then sonicated and emulsified at 20,000 PSI for 4 min at 4°C. The maleimide group on MPB-PEG-DSPE reacted with the thiol group on the peptide to form a thioether linkage. The nanoparticles were ~353 nm in diameter as measured by laser light scattering. The peptide conjugation efficiency was 88% with 870 peptides per nanoparticle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+in+vitro)]

Southworth et al. (14) performed cell-binding assays with VCAM-1-targeted nanoparticles using murine endothelial 2F-2B cells with fluorescence microscopy. The cells were clearly visualized with VCAM-1-targeted nanoparticles but not with non-targeted nanoparticles. Ani-VCAM-1 antibody inhibited the binding of VCAM-1-targeted nanoparticles to the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+rodentia)]

Southworth et al. (14) performed ex vivo MR imaging (^19^F) at 11.7T with kidneys (n = 6) from ApoE^-/-^ and wild-type mice injected with VCAM-1-targeted nanoparticles at 2 h after injection. The ^19^F signal in the ApoE^-/-^ kidneys from mice injected with targeted nanoparticles was 3-fold greater than that observed in the wild-type kidneys from mice injected with targeted nanoparticles. There were 36.6 ± 8.8 x 10^8^ targeted nanoparticles/g versus 9.3 ± 2.2 x 10^8^ non-targeted nanoparticles/g in the ApoE^-/-^ kidneys. On the other hand, the number of nanoparticles was similar in the wild-type kidneys (15.6 and 15.4 x 10^8^/g, respectively). Histoimmunostaining showed that there was a 2-fold greater expression of VCAM-1 in the ApoE^-/-^ kidneys than the wild-type kidneys. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+human)]

No publication is currently available.

## NIH Support

HL073646, CA119342, R01 HL078631-04

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
3 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
4 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
5 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
6 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
7 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
8 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
9 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
10 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
11 Tsourkas A., Shinde-Patil V.R., Kelly K.A., Patel P., Wolley A., Allport J.R., Weissleder R. (2005). In vivo imaging of activated endothelium using an anti-VCAM-1 magnetooptical probe. Bioconjug Chem.
12 Kelly, K.A., M. Nahrendorf, A.M. Yu, F. Reynolds, and R. Weissleder, In Vivo Phage Display Selection Yields Atherosclerotic Plaque Targeted Peptides for Imaging. Mol Imaging Biol, 2006
13 Nahrendorf M., Jaffer F.A., Kelly K.A., Sosnovik D.E., Aikawa E., Libby P., Weissleder R. (2006). Noninvasive vascular cell adhesion molecule-1 imaging identifies inflammatory activation of cells in atherosclerosis. Circulation.
14 Southworth R., Kaneda M., Chen J., Zhang L., Zhang H., Yang X., Razavi R., Lanza G., Wickline S.A. (2009). Renal vascular inflammation induced by Western diet in ApoE-null mice quantified by (19)F NMR of VCAM-1 targeted nanobeacons. Nanomedicine.